# [^99m^Tc]Vasoactive intestinal peptide-aminobutyric acid-Gly-Gly-(D)-Ala-Gly

Chemical name: | [^99m^Tc]Vasoactive intestinal peptide-aminobutyric acid-Gly-Gly-(D)-Ala-Gly
Abbreviated name: | [^99m^Tc]TP3954
Synonym: | [^99m^Tc]VIP
Agent Category: | Peptide
Target: | Vasoactive intestinal peptide receptor
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Proposed structure of ^99m^Tc-TP3654. Aba* = 4-Aminobutyric acid

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=vasoactive+intestinal+peptide+receptors)]

The vasoactive intestinal peptide (VIP) receptors (VIPR) are believed to be involved in the modulation of many physiological processes such as growth, reproduction, digestion, and respiration, as well as the neuroendocrine, cardiovascular, and immune systems, and even cancers (1-4). VIPR have been reported to be expressed by most human carcinomas and hve been detected in more tumors compared with the somatostatin receptors, and the use of these receptors for tumor imaging was suggested (5). The VIP is a hydrophobic peptide (28 amino acids) that was labeled with radioactive iodine (^123^I), and Virgolini et al. used ^123^I-VIP to image human primary tumors and metastases (6). In another investigation, using the same ligand for in vitro studies, Reubi et al. showed that ^123^I-VIP bound to the VIPR in human mesenchymal tumors (7). Based on the ease of availability of radioactive meta-stable technetium (^99m^Tc), Pallela et al. decided to develop and evaluate the use of ^99m^Tc-labeled VIP (^99m^Tc-VIP) for the detection of VIPR in tumors (8).

To use VIP for the detection of tumors, the ligand was derivatized with 4-aminobutyric acid at the carboxy terminus and extended with a Gly-Gly-(D)-Ala-Gly tetrapeptide to facilitate the binding of ^99m^Tc (9). The tissue distribution of ^99m^Tc-VIP (also designated as ^99m^Tc-TP3654) was then studied in nude mice bearing xenograft tumors.

The use of VIP for the treatment of various physiological conditions is under investigation in different clinical trials (http://clinicaltrials.gov/ct2/results?term=vasoactive+intestinal+peptide) approved by the United States Food and Drug Administration.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=vasoactive+intestinal+peptide+synthesis)]

The synthesis of TP3654 was detailed by Pallela et al. (8). Briefly, the peptide was custom synthesized using Wang resin on a peptide synthesizer. TP3654 was cleaved from the resin with 90% trifluoroacetic acid and precipitated with diethyl ether at -20°C. Purification of the peptide was performed with reverse-phase high-performance liquid chromatography (RP-HPLC) on a C_18_ HAIsil column. The various fractions were lyophilized and characterized with ion-spray mass spectrometry.

A lyophilized preparation of TP3654 was used for ^99m^Tc labeling of the peptide (8). The peptide was dissolved in acetate buffer (pH 4.6) and dispensed into glass vials containing tin chloride in hydrochloric acid (HCl) and trisodium phosphate buffer (pH 12.0). The mixture was frozen immediately in an acetone dry ice bath and lyophilized for 2 h. The vials were flushed with nitrogen gas, sealed, and stored at -20°C until used. For labeling with ^99m^Tc, the vials were warmed to 22°C, and sodium ^99m^Tc-pertechnetate in normal saline was added. The mixture was incubated for 15 min, and the pH of the solution was raised to between 6 and 6.5 by the addition of dibasic sodium phosphate solution (pH 5.2). Ascorbic acid was subsequently added as a stabilizer. RP-HPLC analysis of the product was performed on a C_18_ Microbond column (8). The radiochemical yield of the reaction was reported to be >99%, and the labeled compound had a specific activity of 5.36 TBq/mmol (1,450 Ci/mmol). The stability of TP3654 was evaluated in 100-molar excess of di-tolyl phosphate, human serum albumin, and cysteine at 37°C for up to 24 h. After 24 h at this temperature, ~11% of the radioactivity was displaced (nature of the displaced radioactivity (i.e., as ^99m^Tc pertechnetate or as degradation products of TP3654 with bound ^99m^Tc) was not described in the publication) as determined with RP-HPLC, but the colloidal content remained <5% at all times (8).

For in vitro studies the radioactive iodine (^125^I) analogs of VIP and TP3654 were synthesized as described elsewhere (8). The yield of the ^125^I-VIP and ^125^I-TP3654 products was ~90%, and the specific activity of both radiochemicals was ~3.7 TBq/mmol (~1,000 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=vasoactive+intestinal+peptide+in+vitro)]

The displacement of ^125^I-VIP from its receptor was studied with unlabeled VIP and TP3654 (8). Human HT-29 (http://www.biotech.ist.unige.it/cldb/cl5205.html) colon adenocarcinoma cells were incubated at 4°C for 1 h with ^125^I-VIP in the presence or absence of increasing concentrations of unlabeled TP3654 or VIP, respectively. The cells were then washed twice with Tris-HCl buffer (pH 7.5), and radioactivity bound to the cells was counted. Both unlabeled competing ligands (TP3654 and VIP) were reported to displace the iodinated ligand and to have a 50% inhibitory concentration of ~15 nmol/L under these assay conditions. This indicated that the biological activity of TP3654 was similar to its parent compound.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=vasoactive+intestinal+peptide+rodentia)]

The biodistribution of ^99m^Tc-TP3654 was studied in nude mice bearing human colorectal cancer LS174T (http://www.biotech.ist.unige.it/cldb/cl3261.html) xenograft tumors (8). The animals (n = 5 per time point) were injected with the radiochemical, and imaging was performed 4 h or 24 h later. In addition, tissues were removed from the treated animals, weighed, and the associated radioactivity was counted in a gamma counter. For comparison, another group of animals were injected with ^125^I-VIP (n = 5 animals per time point and group) or ^99m^Tc-Gly-Gly(D)-Ala-Gly (prepared as given for ^99m^Tc-TP3654) and treated in the same manner as the animals treated with ^99m^Tc-TP3654. The biodistribution of ^99m^Tc-TP3654 was reported to be distinctly different from that of ^99m^Tc-Gly-Gly-(D)-Ala-Gly as determined by counting radioactivity accumulated in the tissue and also by imaging (8). The ^99m^Tc-TP3654 was reported to be excreted primarily by the kidneys with a low uptake in the liver. The tumor uptake of ^99m^Tc-TP3654 remained constant from 4 h to 24 h (0.24 ± 0.08% and 0.23 ± 0.13%, respectively, of the injected dose (% ID)). At 24 h the tumor/muscle and the tumor/blood ratios for ^99m^Tc-TP3654 were 6.28 ± 3.09 and 1.98 ± 1.44, respectively, and these were significantly higher than the ratios obtained with ^125^I-VIP (0.38 ± 0.56 and 0.88 ± 0.16, respectively). No blocking studies were reported by the investigators.

Using athymic NCr nude mice bearing human LS174T cell tumors, the tissue distribution and efficacy of ^99m^Tc-TP3654 to detect colorectal cancer was compared to that of radioactive indium (^111^In)–labeled D-Phe’-octeroid (^111^In-octeroid) and ^99m^Tc-anti-carcinoembryonic antigen antibodies (^99m^Tc-anti-CEA) (10). The investigators reported that although the tumor uptake of [^99m^Tc]TP3654 was modest (0.21 ± 0.07% ID/g) compared with ^99m^Tc-anti-CEA (3.55 ± 0.5% ID/g), and superior compared to ^111^In-octreotide (0.09 ± 0.02% ID/g), the tissue distribution profile of ^99m^Tc-TP3654 was better than either ^99m^Tc-anti-CEA or ^111^In-octreotide (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+TP3654+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+TP3654+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+TP3654+humans)]

The efficacy of ^99m^Tc-TP3654 for the detection of tumors was investigated in 3 healthy volunteers and 11 volunteers with a history of various cancers (11). Each individual was given a intravenous bolus injection of the radiochemical, and imaging was performed up to 2 h after the injection. Among the cancer patients, all previously known tumors were visualized by imaging within 20 min of the administration of ^99m^Tc-TP3654. The investigators then compared these observations with results that were obtained when ^99m^Tc-methoxyisobutyl isonitrile, computed tomography, magnetic resonance imaging, or histology were used to detect the tumors. A concordance with all the modalities was evident in 9 of the 11 cancer patients, and uptake of the radiochemical by tumors of the cancer patients was rapid. The two remaining patients were positive only with ^99m^Tc-TP3654 (11). Between the two patients, one had a high-grade spindle cell carcinoma in the neck, and the second patient had ductal epithelial hyperplasia in a breast. Both of these tumors are known to express VIPR (12).

In another study with normal human volunteers (n = 4), the investigators reported that ^99m^Tc-TP3654 was cleared rapidly from the blood. ^99m^Tc-TP3654 was reported to be excreted primarily through the kidneys (70%) and the hepatobiliary route (20%) within 24 h of administration (10).

## Supplemental Information

[Disclaimers]

## References

1 Favrais G., Couvineau A., Laburthe M., Gressens P., Lelievre V. (2007). Involvement of VIP and PACAP in neonatal brain lesions generated by a combined excitotoxic/inflammatory challenge. Peptides.
2 Gonzalez-Rey E., Anderson P., Delgado M. (2007). Emerging roles of vasoactive intestinal peptide: a new approach for autoimmune therapy. Ann Rheum Dis.
3 Laburthe M., Couvineau A., Tan V. (2007). Class II G protein-coupled receptors for VIP and PACAP: structure, models of activation and pharmacology. Peptides.
4 Moody T.W., Gozes I. (2007). Vasoactive intestinal peptide receptors: a molecular target in breast and lung cancer. Curr Pharm Des.
5 Reubi J.C. (1995). In vitro identification of vasoactive intestinal peptide receptors in human tumors: implications for tumor imaging. J Nucl Med.
6 Virgolini I., Raderer M., Kurtaran A., Angelberger P., Banyai S., Yang Q., Li S., Banyai M., Pidlich J., Niederle B., Scheithauer W., Valent P. (1994). Vasoactive intestinal peptide-receptor imaging for the localization of intestinal adenocarcinomas and endocrine tumors. N Engl J Med.
7 Reubi J.C., Waser B., Laissue J.A., Gebbers J.O. (1996). Somatostatin and vasoactive intestinal peptide receptors in human mesenchymal tumors: in vitro identification. Cancer Res.
8 Pallela V.R., Thakur M.L., Chakder S., Rattan S. (1999). 99mTc-labeled vasoactive intestinal peptide receptor agonist: functional studies. J Nucl Med.
9 Vanbilloen H.P., Bormans G.M., De Roo M.J., Verbruggen A.M. (1995). Complexes of technetium-99m with tetrapeptides, a new class of 99mTc-labelled agents. Nucl Med Biol.
10 Rao P.S., Thakur M.L., Pallela V., Patti R., Reddy K., Li H., Sharma S., Pham H.L., Diggles L., Minami C., Marcus C.S. (2001). 99mTc labeled VIP analog: evaluation for imaging colorectal cancer. Nucl Med Biol.
11 Thakur M.L., Marcus C.S., Saeed S., Pallela V., Minami C., Diggles L., Le Pham H., Ahdoot R., Kalinowski E.A. (2000). 99mTc-labeled vasoactive intestinal peptide analog for rapid localization of tumors in humans. J Nucl Med.
12 Thakur M.L., Marcus C.S., Saeed S., Pallela V., Minami C., Diggles L., Pham H.L., Ahdoot R., Kalinowski E.A., Moody T. (2000). Imaging tumors in humans with Tc-99m-VIP. Ann N Y Acad Sci.